# ^64^Cu-1,4,7-Triazacyclononane-1,4-diacetate-8-aminooctanoic acid-Gln-Trp-Ala-Val-Gly-His-Leu-Met-NH_2_

Chemical name: | ^64^Cu-1,4,7-Triazacyclononane-1,4-diacetate-8-aminooctanoic acid-Gln-Trp-Ala-Val-Gly-His-Leu-Met-NH_2_
Abbreviated name: | ^64^Cu-NO2A-8-Aoc-BBN[7-14]NH_2_
Synonym:
Agent category: | Peptide
Target: | Gastrin-releasing peptide receptor (GRPR)
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal\contrast: | ^64^Cu
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=4885361), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=61677286) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=2925) for more information about gastrin-releasing peptide receptor.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=BBN+NO2A)]

The amphibian bombesin (BBN or BN, a peptide of 14 amino acids) is an analog of human gastrin-releasing peptide (GRP, a peptide of 27 amino acids) that binds to GRP receptors (GRPR) with high affinity and specificity (1, 2). Both GRP and BBN share an amidated C-terminus sequence homology of seven amino acids, Trp-Ala-Val-Gly-His-Leu-Met-NH_2_. BBN-Like peptides have been shown to induce various biological responses in diverse tissues, including the central nervous system and the gastrointestinal system. They also act as potential growth factors for both normal and neoplastic tissues (3). Specific BBN receptors (BBN-R) have been identified on central nervous system and gastrointestinal tissues and on a number of tumor cell lines (4). The BBN-R superfamily includes at least four different subtypes, namely the GRPR subtype (BB2), the neuromedin B (NMB) receptor subtype (BB1), the BB3 subtype, and the BB4 subtype. The findings of GRPR overexpression in various human tumors, such as breast, prostate, lung, colon, ovarian, and pancreatic cancers, provide opportunities for tumor imaging by designing specific molecular imaging agents to target the GRPR (5, 6).

Prasanphanich et al. (7) used 1,4,7-triazacyclononane-1,4-diacetate (NO2A) as a bifunctional chelator for labeling 8-aminooctanoic acid-Gln-Trp-Ala-Val-Gly-His-Leu-Met-NH_2_ (8-Aoc-BBN[7-14]NH_2_) with ^64^Cu. ^64^Cu-NO2A-8-Aoc-BBN[7-14]NH_2_ has been evaluated as a positron emission tomography (PET) imaging agent of GRPR in nude mice bearing T-47D human breast cancer cells.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=BBN+NO2A+synthesis)]

8-Aoc-BBN[7-14]NH_2_ was prepared with solid-phase peptide synthesis with subsequent addition of NO2A group to form NO2A-8-Aoc-BBN[7-14]NH_2_ (7). ^64^CuCl_2_ was added to a solution of NO2A-8-Aoc-BBN[7-14]NH_2_ in ammonium acetate (pH 7.1). The mixture was heated for 30 min at 70°C. The product, ^64^Cu-NO2A-8-Aoc-BBN[7-14]NH_2_, was purified with high-performance liquid chromatography with a yield of >90% and a radiochemical purity of >99%. The specific activity of ^64^Cu-NO2A-8-Aoc-BBN[7-14]NH_2_ was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=BBN+NO2A+in+vitro)]

Prasanphanich et al. (7) performed in vitro inhibition studies of NO2A-8-Aoc-BBN[7-14]NH_2_ and ^64^Cu-NO2A-8-Aoc-BBN[7-14]NH_2_ in cultured T-47D cells with ^125^I-BBN. The 50% inhibition concentration (IC_50_) values were 5.99 for NO2A-8-Aoc-BBN[7-14]NH_2_ and 7.56 nM for ^64^Cu-NO2A-8-Aoc-BBN[7-14]NH_2_. T-47D cells exhibited a 90% uptake of incubation dose of ^64^Cu-NO2A-8-Aoc-BBN[7-14]NH_2_ within 60 min of incubation at 37°C, indicating cell internalization of the radioligand. More than 90% of the internalized radioactivity remained inside the cells over 90 min of incubation in fresh medium.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=BBN+NO2A+%20rodentia)]

Prasanphanich et al. (7) performed ex vivo biodistribution studies of 0.26 MBq (7 μCi) ^64^Cu-NO2A-8-Aoc-BBN[7-14]NH_2_ in normal mice. The heart, lung, spleen, stomach, muscle, bone, brain, and blood exhibited very little (<0.5% injected dose per gram (ID/g)) of the accumulated conjugate at 1, 4, and 24 h after injection. Pancreatic accumulation was 27.0, 9.1, and 1.4% ID/g at the respective time points. The small intestine showed accumulation of 10.8, 1.9, and 0.4% ID/g, while the large intestine accumulated 2.1, 15.1, and 0.5% ID/g at these time points. Radioactivity accumulation in the kidney was 2.9, 0.7, and 0.4% ID/g, respectively. Accumulation in the liver was 1.5, 1.1, and 0.7% ID/g, respectively. The urinary excretion was 63, 77, and 81% ID. Administration of D-lysine (15 mg/mouse) had little effect on the biodistribution of ^64^Cu-NO2A-8-Aoc-BBN[7-14]NH_2_. Ex vivo biodistribution studies of ^64^Cu-NO2A-8-Aoc-BBN[7-14]NH_2_ were performed in nude mice bearing T-47D xenografts. Tumor accumulation at these time points was 2.27 ± 0.08, 1.35 ± 0.14, and 0.28 ± 0.07% ID/g, while the biodistribution pattern in the other tissues was similar to that of the normal mice. The tumor/muscle ratios were 9.5, 7.5, and 5.6 at 1, 4, and 24 h after injection, respectively. Pretreatment of excess BBN[1-14] (100 µg/mouse) inhibited the tumor accumulation by 75%, whereas the accumulation in the pancreas, small intestine, and large intestine was inhibited by ~90% with little effect in the other tissues at 1 h after tracer injection. PET imaging in nude mice bearing T-47D xenografts was performed with 189 MBq (5.1 mCi) ^64^Cu-NO2A-8-Aoc-BBN[7-14]NH_2_ at 24 h after injection. The tumors were clearly visualized, as were the pancreas, liver, and kidneys.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=BBN+NO2A+and%20%28pig%20or%20dog%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=BBN+NO2A+and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=BBN+NO2A+human)]

No publication is currently available.

## References

1 Gonzalez N., Moody T.W., Igarashi H., Ito T., Jensen R.T. (2008). Bombesin-related peptides and their receptors: recent advances in their role in physiology and disease states. Curr Opin Endocrinol Diabetes Obes.
2 Bertaccini G. (1976). Active polypeptides of nonmammalian origin. Pharmacol Rev.
3 Chung D.H., Evers B.M., Beauchamp R.D., Upp J.R., Rajaraman S., Townsend C.M., Thompson J.C. (1992). Bombesin stimulates growth of human gastrinoma. Surgery.
4 Benya R.V., Kusui T., Pradhan T.K., Battey J.F., Jensen R.T. (1995). Expression and characterization of cloned human bombesin receptors. Mol Pharmacol.
5 Reubi J.C., Wenger S., Schmuckli-Maurer J., Schaer J.C., Gugger M. (2002). Bombesin receptor subtypes in human cancers: detection with the universal radioligand (125)I-[D-TYR(6), beta-ALA(11), PHE(13), NLE(14)] bombesin(6-14). Clin Cancer Res.
6 Smith C.J., Volkert W.A., Hoffman T.J. (2005). Radiolabeled peptide conjugates for targeting of the bombesin receptor superfamily subtypes. Nucl Med Biol.
7 Prasanphanich A.F., Retzloff L., Lane S.R., Nanda P.K., Sieckman G.L., Rold T.L., Ma L., Figueroa S.D., Sublett S.V., Hoffman T.J., Smith C.J. (2009). In vitro and in vivo analysis of [(64)Cu-NO2A-8-Aoc-BBN(7-14)NH(2)]: a site-directed radiopharmaceutical for positron-emission tomography imaging of T-47D human breast cancer tumors. Nucl Med Biol.